# Mouse anti-cMet monoclonal antibody linked to gadolinium diethylenetriamine pentaacetic acid conjugated to biotinylated bovine serum albumin

Chemical name: | Mouse anti-cMet monoclonal antibody linked to gadolinium diethylenetriamine pentaacetic acid conjugated to biotinylated bovine serum albumin | [image]
Abbreviated name: | Anti-c-Met-Gd-DTPA-albumin | [image]
Synonym: | Anti-c-Met MAb-Gd-DTPA-biotinylated BSA | [image]
Agent Category: | Antibody | [image]
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | [image]
Target Category: | Receptor | [image]
Method of detection: | Magnetic resonance imaging (MRI) | [image]
Source of signal / contrast: | Gd | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of anti-c-Met-Gd-DTPA-albumin Modified from (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+c+Met+Gd+albumin)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (2). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways, leading to initiation of the various cell processes (3). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or mutation promotes the development of a neoplastic cell phenotype (3). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (4), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (5). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration.

Because the overexpression of HGF and c-Met in malignant gliomas indicates a poor prognosis for the patient, c-Met is a tumor marker of interest for the detection and diagnosis of this disease (1, 6). Although brain lesions are quite easily detected when a contrast agent (CA) is used in conjunction with magnetic resonance imaging (MRI), this technique cannot determine the molecular basis for development of the lesion (1). However, an antibody or a ligand can be used to target a gadolinium (Gd)-based CA for use with MRI to detect and possibly quantify a specific cell-surface component or antigen that may have an important role in the development of a malignancy. Using this approach, investigators were successful in using Gd linked to diethylenetriamine pentaacetic acid and conjugated to a folate-containing dendrimer to quantify folate receptor expression in xenograft tumors on mice (7). In another study, SCID mice bearing xenograft tumors expressing the Her-2/neu receptor were pre-exposed to a biotinylated anti–Her-2/neu monoclonal antibody (MAb), and the animals were subsequently treated with an avidin-Gd-DTPA conjugate (8). Using MRI, the investigators obtained tumor images and determined the level of Her-2/neu receptor expression in the tumor tissue. On the basis of these studies, Towner et al. evaluated the use of Gd-DTPA-albumin coupled to an anti-c-Met MAb (anti-c-Met-Gd-DTPA-albumin) for the visualization of c-Met overexpression in an intracranial rat glioma model (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+albumin+synthesis)]

The synthesis of anti-c-Met-Gd-DTPA-albumin has been discussed in detail by Towner et al. (1). Briefly, biotinylated bovine serum albumin (BSA) was first linked to Gd-DTPA to obtain biotin-BSA-Gd-DTPA (the number of Gd attached to each molecule of biotib-BSA was not reported), and this complex was then conjugated to a mouse anti-c-Met MAb (http://www.scbt.com/datasheet-8057-met-b-2-antibody.html) to obtain anti-c-Met-Gd-DTPA-albumin, the MRI CA. Biotinylated BSA was used to facilitate detection of anti-c-Met-Gd-DTPA-albumin with immunofluorescence staining using Cy3-streptavidin. The final product was freeze-dried and stored at 4°C until required. The freeze-dried anti-c-Met-Gd-DTPA-albumin was reconstituted in phosphate-buffered saline (pH not reported) before treating the animals. Using a similar procedure, rat IgG (http://www.4adi.com/objects/catalog/product/extras/20005-1-5-10.pdf)-biotin-BSA-Gd-DTPA was also prepared for use as a control CA. The stability of the various CAs after reconstitution was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+DTPA+albumin+in+vitro)]

The overexpression of c-Met in rat gliomas compared with normal rat brain tissue was detected with Western blot analysis by Towner et al. (1). After immunofluorescence staining with Cy3-streptavidin, an increased fluorescence was observed in the gliomas compared with the normal brain tissue, which confirmed the overexpression of c-Met in the tumors as noted with the Western blots (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+DTPA+rodentia)]

Rats (the number of animals used was not reported) bearing gliomas were treated with the control IgG CAs, the c-Met–directed CAs, or the Gd-DTPA-BSA CAs, and T_1_-weighted images of the animal brains were obtained before and 3 h after injection of the CAs through the tail vein (1). Several ^1^H-MRI image slices were taken in the transverse plane with a multi-spin echo, multi-slice sequence using a repetition time of 2.4 s and echo times of 17.4 (T_1_-weighted) and 63.9 (T_2_-weighted) (1). The T_1_-weighted images revealed the anatomical details of the brain, whereas the T_2_-weighted images provided contrast to detect the tumors. A decrease in T_1_ relaxation with a simultaneous increase in the MRI signal intensity indicated specific binding of anti-c-Met-Gd-DTPA-albumin to areas within the glioma tumors.

On the basis of the T_1_ maps obtained 3 h after treatment and the signal intensities from various regions of the brain, it was reported that a significantly increased signal intensity and concentration (P = 0.01–0.05) of the c-Met–specific CA on the glioma tumor periphery and interior of animals treated with anti-c-Met-Gd-DTPA-albumin was observed compared with the signal intensity and concentration of the CAs in tumors obtained from animals treated with Gd-DTPA-BSA or control IgG CAs and the normal brain. The binding specificity of anti-c-Met-Gd-DTPA-albumin to the tumors was confirmed with immunofluorescence staining. In addition, the T_1_ values for the tumors were reported to decrease over a 3-h period with an increase in the contrast signal during that time, however during the same period the T_1_ and the contrast signal values returned to precontrast treatment levels in the normal brain tissue. No blocking studies were reported.

From these studies, the investigators concluded that anti-c-Met-Gd-DTPA-albumin could be used for the detection of c-Met in rodents under in vivo conditions (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+DTPA+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+DTPA+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+DTPA+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some studies presented in this chapter were funded by a National Institutes of Health grant 5RO3CA121359-2.

## References

1 Towner R.A., Smith N., Doblas S., Tesiram Y., Garteiser P., Saunders D., Cranford R., Silasi-Mansat R., Herlea O., Ivanciu L., Wu D., Lupu F. (2008). In vivo detection of c-Met expression in a rat C6 glioma model. J Cell Mol Med.
2 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
3 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
4 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
5 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
6 Lamszus K., Laterra J., Westphal M., Rosen E.M. (1999). Scatter factor/hepatocyte growth factor (SF/HGF) content and function in human gliomas. Int J Dev Neurosci.
7 Konda S.D., Aref M., Wang S., Brechbiel M., Wiener E.C. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. Magma.
8 Artemov D., Mori N., Ravi R., Bhujwalla Z.M. (2003). Magnetic resonance molecular imaging of the HER-2/neu receptor. Cancer Res.